# ^99m^Tc-Labeled anti-receptor for advanced glycation endproducts polyclonal antibody F(ab’)_2_ fragments

Chemical name: | ^99m^Tc-Labeled anti-receptor for advanced glycation endproducts polyclonal antibody F(ab’)_2_ fragments | [image]
Abbreviated name: | ^99m^Tc-anti-RAGE pF(ab’)_2_ | [image]
Synonym: | ^99m^Tc-anti-RAGE F(ab’)_2_ | [image]
Agent Category: | Antibodies | [image]
Target: | Receptor for advanced glycation endproducts (RAGE) | [image]
Target Category: | Receptors | [image]
Method of detection: | Planar imaging, single-photon emission computed tomography (SPECT) | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of RAGE.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=AGE+and+RAGE)]

The ^99m^Tc-labeled anti-receptor for advanced glycation endproducts (RAGE) polyclonal antibody F(ab’)_2_ fragment, abbreviated as ^99m^Tc-anti-RAGE pF(ab’)_2_ or ^99m^Tc-anti-RAGE F(ab’)_2_, is a radiotracer developed by Tekabe et al. for imaging atherosclerotic lesions by targeting highly expressed RAGE (1). RAGE is a 35-kDa transmembrane receptor of the immunoglobulin (Ig) superfamily (1, 2).

RAGE has one V domain, two C domains, one transmembrane domain, and one cytoplasmic tail. The V domain consists of two N-glycosylation sites and is responsible for extracellular ligand binding. RAGE exists in three forms: full-length, membrane-bound, and soluble (1-3). The soluble Isoform of the RAGE protein, which lacks the transmembrane and the signalling domain are thought to counteract the detrimental action of the full-length RAGE. Under physiological conditions, RAGE is expressed at low levels in a variety of cells in a regulated manner, but RAGE is highly expressed in a series of age- and diabetes-related chronic inflammatory diseases and cancer (4-7). The advanced glycation endproducts (AGEs) are the major ligands of RAGE. AGEs are a heterogeneous group of peptides and proteins derived from non-enzymatic glycosylation processes (2, 4). Large amounts of AGEs is formed through metabolism and aging, and this establishes a positive feedback cycle under pathological conditions such as diabetes (1, 3, 8). The interaction between AGEs and RAGE affects almost all types of cells and molecules and results in pro-inflammatory gene activation (7, 9). The pathological effects induced by the AGEs/RAGE interaction include increasing vascular permeability, inhibiting vascular dilation, inducing cytokine secretion, enhancing oxidative stress, and modulating cell response to exogenous growth factors. Understanding of the AGEs/RAGE interaction is crucial to develop new treatment regimens for age- and diabetes-related conditions and cancer (3, 9).

In the case of atherosclerosis, AGEs are formed at a high level (10). RAGE itself is expressed in nearly all cell types pertinent for the development and progression of atherosclerotic plaque. The AGEs/RAGE interaction leads to diabetic vascular complications and augments atherosclerotic plaque development and progression (7, 8). In a proof-of-concept study of whether the expression level of RAGE could be detected and thus used as a marker of atherosclerosis, Tekabe et al. developed an anti-RAGE polyclonal antibody F(ab’)_2_ fragment and demonstrated the feasibility of using ^99m^Tc-anti-RAGE pF(ab’)_2_ for the noninvasive detection of RAGE in the atherosclerotic plaques in apolipoprotein E–null (ApoE^–/–^) mouse model (1). The major limitation to this study is that polyclonal antibody fragments and planar imaging modality were used (1). Polyclonal antibodies usually have less specificity and higher background signal compared with monoclonal antibodies. Planar imaging systems have a lower spatial resolution than tomographic imaging systems such as single-photon emission computed tomography.

### Related Resource Links:

- Gene information of RAGE in GenBank (http://www.ncbi.nlm.nih.gov/gene/177)
- Article on RAGE in OMIM (http://www.ncbi.nlm.nih.gov/omim/600214)
- AGE substance in PubChem (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?sid=53787607&loc=es_rss)
- MICAD chapter on ^99m^Tc-anti-RAGE mF(ab’)_2_ (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20008983)]

Tekabe et al. described in detail the production and radiolabeling of the polyclonal antibody F(ab’)_2_ fragment (1). Briefly, the peptide Ac-NRRGKEVKSNYRVRVYQIC-amide on the basis of the V domain of RAGE was synthesized and injected into rabbits. The serum was retrieved, and the IgG was prepared and affinity-purified. The F(ab')_2_ fragments were generated with pepsin digestion of the intact antibody. ^99m^Tc-Labeling of the fragments was performed with diethylenetriamine pentaacetic acid (DTPA) modification, followed by reaction with ^99m^TcO_4_- in SnCl_2_ in 0.1 N HCl. The specific activity of the radiotracer ^99m^Tc-anti-RAGE pF(ab’)_2_ was 1.8 ± 0.34 MBq/µg (48.7 ± 9.3 µCi/µg) protein and the radiochemical purity was 95 ± 1.6%. The radiolabeling yield was not reported. Nonspecific control IgG was prepared from nonimmune rabbit serum, fragmented into F(ab')_2_, and coupled to DTPA for ^99m^Tc labeling as described above.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20008983)]

Immunoreactivities of the intact antibody and antibody fragment were tested against soluble RAGE (1). The antibody concentration for the DTPA-modified F(ab')_2_ fragment, given 50% of maximum binding, was 0.9 µg/ml, which was equivalent to 9 × 10^–9^ mol/L or apparent affinity of 0.11 × 10^9^ L/mol. The concentration for the unmodified anti-RAGE IgG was 0.8 µg/ml, which was equivalent to 8 × 10^–9^ mol/L or apparent affinity of 0.12 × 10^9^ L/mol.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20008983)]

Tekabe et al. measured the blood-pool clearance of ^99m^Tc-anti-RAGE pF(ab’)_2_ in male C57BL/6 mice to determine the optimal time for imaging (1). The clearance was biexponential, with the half-life equal to 15 min for the first (fast) component and 7 h for the second (slower) component. Therefore, Tekabe et al. performed planar γ imaging at 4 h after tracer injection in atherosclerotic model of male ApoE^–/–^ mice (n = 13). Corresponding wild-type male C57BL/6 mice (n = 4) on normal chow were used as controls.

Planar γ imaging showed focal uptake for the ^99m^Tc-anti-RAGE pF(ab’)_2_ in the atherosclerotic lesions in the proximal aorta (n = 6 mice), but no uptake for the nonspecific IgG F(ab’)_2_ (n = 6 mice). Control C57BL/6 mice injected with ^99m^Tc-anti-RAGE pF(ab’)_2_ also showed no localization of the radiotracer in the proximal aorta (no lesions at gross examination). There was a significant difference between the three groups of mice in terms of tracer uptake in proximal aorta relative to whole body (Friedman; χ^2^ = 12.83; P = 0.0016) (1). This value was 1.03% for ^99m^Tc-anti-RAGE pF(ab’)_2_, 0.17% for nonspecific IgG F(ab’)_2_ in the experimental ApoE^–/–^ mice, and 0.31% for ^99m^Tc-anti-RAGE pF(ab’)_2_ in the control C57BL/6 mice at 4 h after injection. Ex vivo counting confirmed the difference for the uptake in the proximal aorta among the three groups of mice (χ^2^ = 9.613; P = 0.0082) (1). Aortic uptakes were 1.76% and 0.13% injected dose per gram tissue (ID/g) in the ApoE^–/–^ mice receiving ^99m^Tc-anti-RAGE pF(ab’)_2_ and nonspecific IgG F(ab’)_2_, respectively, and this value was 0.39% ID/g in the control C57BL/6 mice receiving ^99m^Tc-anti-RAGE pF(ab’)_2_. In the ApoE^–/–^ mice injected with ^99m^Tc-anti-RAGE pF(ab’)_2_, a significant difference for the radiotracer uptake was also observed between thoracic organs (aortic lesions, heart (0.50% ID/g), and lungs (0.90% ID/g)) (χ^2^ = 8; P = 0.0183). Histology and immunohistochemical staining of the proximal aorta confirmed formation of atherosclerotic lesions and uptake of the radiotracer in the lesions expressing RAGE (1). In biodistribution studies at 5–6 h after injection, the highest uptake was observed in the subdiaphragmatic organs (particularly in the liver and spleen) for both ^99m^Tc-anti-RAGE pF(ab’)_2_ and nonspecific IgG F(ab’)_2_ as observed on the in vivo scans (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Tekabe Y., Li Q., Rosario R., Sedlar M., Majewski S., Hudson B.I., Einstein A.J., Schmidt A.M., Johnson L.L. (2008). Development of receptor for advanced glycation end products-directed imaging of atherosclerotic plaque in a murine model of spontaneous atherosclerosis. Circ Cardiovasc Imaging.
2 Yan S.F., Ramasamy R., Schmidt A.M. (2010). The RAGE axis: a fundamental mechanism signaling danger to the vulnerable vasculature. Circ Res.
3 Sourris K.C., Forbes J.M. (2009). Interactions between advanced glycation end-products (AGE) and their receptors in the development and progression of diabetic nephropathy - are these receptors valid therapeutic targets. Curr Drug Targets.
4 Daroux M., Prevost G., Maillard-Lefebvre H., Gaxatte C., D'Agati V.D., Schmidt A.M., Boulanger E. (2010). Advanced glycation end-products: implications for diabetic and non-diabetic nephropathies. Diabetes Metab.
5 Abe R., Yamagishi S. (2008). AGE-RAGE system and carcinogenesis. Curr Pharm Des.
6 Fang F., Lue L.F., Yan S., Xu H., Luddy J.S., Chen D., Walker D.G., Stern D.M., Schmidt A.M., Chen J.X., Yan S.S. (2010). RAGE-dependent signaling in microglia contributes to neuroinflammation, Abeta accumulation, and impaired learning/memory in a mouse model of Alzheimer's disease. FASEB J.
7 Nienhuis H.L., Westra J., Smit A.J., Limburg P.C., Kallenberg C.G., Bijl M. (2009). AGE and their receptor RAGE in systemic autoimmune diseases: an inflammation propagating factor contributing to accelerated atherosclerosis. Autoimmunity.
8 Walcher D., Marx N. (2009). Advanced glycation end products and C-peptide-modulators in diabetic vasculopathy and atherogenesis. Semin Immunopathol.
9 Ramasamy R., Yan S.F., Schmidt A.M. (2009). RAGE: therapeutic target and biomarker of the inflammatory response--the evidence mounts. J Leukoc Biol.
10 Tekabe Y., Luma J., Einstein A.J., Sedlar M., Li Q., Schmidt A.M., Johnson L.L. (2010). A novel monoclonal antibody for RAGE-directed imaging identifies accelerated atherosclerosis in diabetes. J Nucl Med.